# ^125^I-Radioiodinated tyrosine-folate and tyrosine-click-folate

Chemical name: | ^125^I-Radioiodinated tyrosine-folate and tyrosine-click-folate | [image]
Abbreviated name: | [^125^I]-2 and [^125^I]-4 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Folate receptor (FR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of [^125^I]-2 and [^125^I]-4

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=folate%20receptor%20and%20folic%20acid%20and%20imaging)]

^125^I-Radioiodinated tyrosine-folate ([^125^I]-2) and tyrosine-click-folate ([^125^I]-4) are two folic acid conjugates synthesized by Reber et al. for imaging tumors by targeting folate receptor (FR) (1).

FR is a well-established target for molecular imaging and therapy. This receptor exhibits some favorable features as a target, such as high affinity for exogenous folate conjugates (K_d_ = ~100 pM), overexpression in a variety of human cancers, mediation of folate conjugates into cells, and self-recycling (2-4). In addition, conjugation of imaging labels via the γ-carboxyl group of folate has no apparent effect on its binding affinity to FR. However, FR expresses at a relatively high density on tumor cell surface (1–3 million FR/cell), and the folate-FR binding can be saturated rapidly. FR also expresses on the luminal side of proximal tubule cells in kidneys and is accessible to filtered radiofolates (5, 6). For most radiofolates, high renal accumulation (tumor/kidney ratio = ~0.1) and the resulting damage to kidneys are constant concerns in radiotherapy (1, 7).

Radioiodination of tyrosine residues is a common strategy for efficient radiolabeling of proteins and peptides (1, 4). The instability of radioiodinated tyrosine constructs as a consequence of in vivo deiodination is generally regarded as a disadvantage for radiopharmaceutical applications. However, studies have shown that the tumor/kidney ratios of radioiodinated conjugates are often higher than those of conjugates labeled with other radionuclides (8). The higher tumor/kidney ratios are considered to be due to partial deiodination of the radioiodinated conjugates.

Reber et al. designed two radioiodinated folic acid conjugates, [^125^I]-2 and [^125^I]-4, based on the hypothesis that radioiodinated folate conjugates would exhibit favorable properties, similar to those found with other radioiodinated conjugates (1) and the partial deiodination of the radioiodinated folate conjugates might result in a quick clearance of the released iodide via kidneys and thus lead to improved tumor/kidney ratios. The findings obtained by Reber et al. confirm the hypothesis and indicate that the two radiofolates are potentially valuable for imaging applications (1). The radiofolate [^131^I]-4 was also tested in combination with Pemetrexed (PMX), a multitargeted antifolate drug (7), for therapeutic purposes. This chapter summarizes the data obtained with [^125^I]-2 and [^125^I]-4.

### Related Resource Links:

Folate receptor–targeted imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=folate+receptor+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=folate%20receptor) and protein (http://www.ncbi.nlm.nih.gov/protein?term=folate%20receptor) sequences of folate receptor

Bioassays of folate receptor (http://www.ncbi.nlm.nih.gov/pcassay/?term=folate%20receptor) in PubChem

Folate receptor–related compounds (http://www.ncbi.nlm.nih.gov/pcsubstance?term=folate%20receptor) in Pubchem

Folate receptor–related clinical trials (http://clinicaltrials.gov/ct2/results?term=folate+receptor) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22509996)]

Reber et al. described the synthesis of tyrosine-folate (compound 1), iodo-tyrosine-folate (compound 2), tyrosine-click-folate (compound 3), and iodo-tyrosine-click-folate (compound 4) in detail (1). The overall yield was ~10% for compound 1 and ~5% for compound 2. Conjugation of the tyrosine moiety of compounds 1 and 2 with “click chemistry” resulted in compounds 3 and 4, respectively, with an overall yield of ~25% for compound 3 and ~14% for compound 4. All compounds were obtained with >95% purity as confirmed with high-performance liquid chromatography (HPLC). Compounds 1 and 3 were radiolabeled with [^125^I]-iodine and [^131^I]-iodine to obtain [^125^I]-2 and [^125/131^I]-4. The specific activities for [^125^I]-iodine and [^131^I]-iodine were 78.6 MBq/nmol (2.12 mCi/nmol) and >24.2 MBq/nmol (0.65 mCi/nmol), respectively. [^125^I]-2 (retention time (R_t_) ≈ 14.4 min) and [^125/131^I]-4 (R_t_ ≈ 15.7 min) were separated from traces of free iodide (R_t_ ≈ 2.9 min) and cold precursor 1 (R_t_ ≈ 12.4 min) or 3 (R_t_ ≈ 13.9 min) with HPLC. Compounds 2 and 4 were used as reference compounds in the experiments.

The radiochemical yields were >97% for both [^125^I]-2 and [^125/131^I]-4. The actual experimental specific activities of [^125^I]-2 and [^125/131^I]-4 were not reported. For in vitro and in vivo experiments, the radiofolates were diluted in phosphate-buffered saline (PBS) at pH 7.4. The octanol/PBS distribution coefficient (log D value) for [^125^I]-2 was slightly higher (−2.87 ± 0.02) than that for [^125^I]-4 (−3.13 ± 0.07), indicating that [^125^I]-4 is more hydrophilic than [^125^I]-2.

The in vitro stabilities of [^125^I]-2 and [^125^I]-4 were determined in mouse and human plasma and in mouse liver microsomes. During the incubation period of 7 days in both mouse and human plasma at 37°C, HPLC analysis always showed only one single peak, with an integrated area of 100% and a retention time that corresponded to the retention times for [^125^I]-2 and [^125^I]-4, indicating no deiodination or decomposition of [^125^I]-2 and [^125^I]-4. In murine liver microsomes, [^125^I]-2 and [^125^I]-4 exhibited no deiodination over a time period of 24 h in contrast to [^125^I]iodo-l-tyrosine, which was almost completely deiodinated within 30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22509996)]

Reber et al. analyzed the cell uptake and binding affinities of [^125^I]-2 and [^125^I]-4 with cultured KB cells (human cervix carcinoma), IGROV-1 and SKOV-3 cells (both are human ovarian adenocarcinoma cells), and PC-3 cells (human prostate carcinoma) (1). KB cells are known to express high levels of FR, whereas IGROV-1 and SKOV-3 cells express lower levels of FR. PC-3 cells do not express FR and were used as a negative control.

Cell uptake studies were performed with KB cells. The results showed that [^125^I]-2 and [^125^I]-4 had similar characteristics. The maximal amount of uptake was reached after 90–120 min incubation at 37°C. The internalized fraction for both radiofolates accounted for 25%–30% of total cell uptake (sum of FR-bound radiofolates on the cell surface and internalized fraction). Co-incubation of [^125^I]-2 or [^125^I]-4 with excess folic acid inhibited uptake for [^125^I]-2 and [^125^I]-4 to <0.1% of the total added radioactivity.

Relative binding affinities were determined with a competition assay with ^3^H-folic acid and the nonradioactive reference compounds 2 and 4. The binding affinity of folic acid was set to 1.0, and a relative affinity value of 1.0 implies that the test compound has an affinity for FR equal to that of folic acid. Likewise, values <1.0 reflect a weaker affinity, and values >1.0 reflect a stronger affinity. Compounds 2 and 4 had a relative binding affinity of 0.78 and 0.67, respectively.

Reber et al. also analyzed cell viability after incubation of the cells with [^131^I]-4 (5 MBq/mL (0.14 mCi/mL)) (1). In the absence of folic acid, [^131^I]-4 reduced the viabilities of FR-positive KB, IGROV-1, and SKOV-3 cells to 4.5%, 15.3%, and 27.4% of the viabilities of the untreated control cells, respectively. However, in the presence of excess folic acid to block FR, the viabilities of these cells were not affected by [^131^I]-4 at the same radioactivity concentration. In addition, no reduction of the cell viability was observed with the same amount of [^131^I]-4 in the control experiments performed with FR-negative PC-3 cells. The half-maximal inhibitory concentrations of [^131^I]-4 were 0.39 ± 0.03 (10.54 ± 0.81), 0.95 ± 0.05 (25.68 ± 1.35), and 1.22 ± 0.09 (32.97 ± 2.43) MBq/mL (µCi/mL) for KB, IGROV-1, and SKOV-3 cells, respectively. The incubation of KB cells with PMX (1 μM) for 4 h and 24 h reduced tumor cell viability to 80% and 50% of the cell viability of the untreated controls, respectively. Application of [^131^I]-4 at a concentration of 0.01 MBq/mL (0.27 µCi/mL) did not affect tumor cell viability if applied as a single agent for 4 h. However, if this radioactivity concentration was applied in combination with PMX (1 μM), it resulted in an enhanced inhibitory effect, decreasing cell viability to 72% (after 4 h) and 23% (after 24 h) compared with untreated controls.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=22509996)]

Biodistribution of [^125^I]-2 and [^125^I]-4 was investigated in CD-1 Foxn-1/nu mice (n = 6–8) (1). Animals were fed a folate-deficient rodent diet starting 5 days before KB cell inoculation. [^125^I]-2 and [^125^I]-4 were given to mice via tail vein injection (0.2 MBq (5.41 µCi)). Potassium iodide dissolved in PBS was injected intraperitoneally (4 mg) 1 h before the radioactive agents. Animals were euthanized at 1, 4, or 24 h after administration of the radiofolate. The radioactivity in organs was recorded as the percentage of the injected dose per gram of tissue weight (% ID/g). Blocking experiments were performed 4 h after coinjection with excess folic acid (100 μg). The results showed that both [^125^I]-2 and [^125^I]-4 accumulated in FR-positive KB tumor xenografts and in kidneys (Tables 1 and 2).

Table 1: Biodistribution data of [^125^I]-2 at different time points after injection

Tissues | 1 h | 4 h | 24 h | 4 h (FA)^1^ | 4 h (KI)^2^
Blood | 3.00 ± 0.56 | 2.15 ± 0.42 | 0.09 ± 0.02 | 2.25 ± 1.00 | 2.71 ± 0.52
Kidneys | 18.33 ± 2.47 | 9.80 ± 1.67 | 0.85 ± 0.06 | 1.79 ± 0.58 | 8.66 ± 1.86
Liver | 16.53 ± 1.20 | 2.74 ± 0.45 | 0.09 ± 0.01 | 0.83 ± 0.32 | 2.90 ± 0.63
Thyroid | 261 ± 67 | 1059 ± 184 | 2830 ± 1272 | 868 ± 367 | 13.74 ± 5.01
Tumor | 4.42 ± 0.66 | 3.43 ± 0.28 | 1.25 ± 0.18 | 1.65 ± 0.61 | 4.03 ± 0.22
Tumor/blood | 1.48 ± 0.18 | 1.65 ± 0.41 | 14.38 ± 3.66 | 0.74 ± 0.04 | 1.53 ± 0.30
Tumor/liver | 0.27 ± 0.04 | 1.28 ± 0.23 | 14.45 ± 1.88 | 1.98 ± 0.18 | 1.43 ± 0.24
Tumor/kidney | 0.24 ± 0.03 | 0.36 ± 0.06 | 1.47 ± 0.14 | 0.90 ± 0.09 | 0.48 ± 0.09

^1^FR blockade with folic acid (FA, 100 μg).

^2^Thyroid blockade with potassium iodide (KI, 4 mg).

Table 2: Biodistribution data of [^125^I]-4 at different time points after injection

Tissues | 1 h | 4 h | 24 h | 4 h (FA)^1^ | 4 h (KI)^2^
Blood | 0.10 ± 0.01 | 0.18 ± 0.15 | 0.01 ± 0.00 | 0.03 ± 0.00 | 0.08 ± 0.01
Kidneys | 19.12 ± 0.58 | 16.44 ± 2.64 | 7.10 ± 1.44 | 0.08 ± 0.00 | 17.84 ± 2.60
Liver | 0.28 ± 0.08 | 0.15 ± 0.03 | 0.02 ± 0.00 | 0.02 ± 0.00 | 0.16 ± 0.03
Thyroid | 8.36 ± 1.77 | 10.81 ± 4.99 | 47.59 ± 28.07 | 9.53 ± 8.10 | 2.47 ± 0.56
Tumor | 2.36 ± 0.05 | 2.28 ± 0.46 | 1.92 ± 0.24 | 0.03 ± 0.01 | 2.53 ± 0.39
Tumor/blood | 23.21 ± 2.17 | 17.41 ± 9.66 | 286.75 ± 53.44 | 1.08 ± 0.47 | 30.93 ± 6.87
Tumor/liver | 8.73 ± 2.13 | 15.19 ± 3.99 | 84.82 ± 12.71 | 2.20 ± 0.96 | 15.78 ± 4.33
Tumor/kidney | 0.12 ± 0.00 | 0.14 ± 0.02 | 0.27 ± 0.05 | 0.41 ± 0.15 | 0.14 ± 0.02

^1^FR blockade with folic acid (FA, 100 μg).

^2^Thyroid blockade with potassium iodide (KI, 4 mg).

The tumor uptake of [^125^I]-2 was higher than the uptake of [^125^I]-4 at 1 h after injection (P = 0.02). However, the tumor retention over time was superior for [^125^I]-4 compared to [^125^I]-2. Coinjection of excess folic acid (4 h after injection) reduced tumor uptake to <2% of the uptake of the control values for [^125^I]-4 but only to 48% for [^125^I]-2. The radioactivity in the kidneys for both [^125^I]-2 and [^125^I]-4 was high at 1 h after injection; however, radioactivity reduced significantly (P < 0.05) at 4 and 24 h after injection. Preinjection of PMX resulted in a significantly reduced uptake of [^125^I]-4 in the kidneys (P < 0.05), while uptake in the tumor xenografts was largely retained. The radioactivity in the liver was high for [^125^I]-2 (>16% and >2% ID/g at 1 h and 4 h after injection) but was almost negligible for [^125^I]-4 (<0.3% and <0.2% ID/g at 1 h and 4 h after injection). In the thyroid glands, large amounts of radioactivity (>1,000% ID/g at 4 h after injection) were found for [^125^I]-2, whereas a >10-fold lower accumulation was observed for [^125^I]-4 at the same time point. Intraperitoneal administration of potassium iodide 1 h before administration of the radiotracer significantly (P < 0.05) reduced the uptake of iodide in the thyroid glands at 4 h after injection ([^125^I]-2, 13.74 ± 5.01% ID/g; [^125^I]-4, 2.53 ± 0.39% ID/g). In the gastrointestinal tract, the radioactivity was comparable for both [^125^I]-2 and [^125^I]-4 (4.5% ID/g at 1 h after injection).

Biodistribution studies were also performed with [^125^I]-4 in combination with preinjection of variable doses of PMX (1 h before injection of [^125^I]-4). Nonradioactive potassium iodide was also injected intraperitoneally (4 mg) 1 h before injection of [^125^I]-4. Biodistribution data obtained at 4 h after [^125^I]-4 injection showed that the tumor uptake was slightly reduced after administration of the highest dose (400 µg) of PMX (1.15 ± 0.17% ID/g, P = 0.08), whereas almost no tumor uptake reduction was observed after administration of 50% of the PMX dose (P = 0.64) and 25% of the PMX dose (P = 0.19). In contrast, the radioactivity in the kidneys was significantly reduced after administration of PMX in a dose-dependent manner (P = 0.01). Thus, by using the highest dose of PMX, the tumor/kidney ratio could be improved >10-fold without significant changes in the tumor/blood, tumor/liver, or tumor/muscle ratio.

Metabolite studies were performed in female Balb/c mice (n = 2/time point). Animals were fed a folate-deficient rodent diet starting 5 days before the experiments. All mice received an intraperitoneal injection of potassium iodide (4 mg) 1 h before injection of ~5 MBq (0.135 mCi (~64 pmol)) [^125^I]-2 or [^125^I]-4. Urine and blood samples were taken 5 min and 30 min after injection of the radiotracer. The analysis of blood samples confirmed greater deiodination of [^125^I]-2 compared to that of [^125^I]-4. As a consequence, a high concentration of free [^125^I]-iodide was found in the blood samples from mice injected with [^125^I]-2 but not in blood samples from mice that received [^125^I]-4. Intact [^125^I]-2 was not detectable in urine samples. In contrast, almost the whole radioactive fraction of [^125^I]-4 in the urine samples taken at 5 min after injection was intact, and only a small amount (~10%) was free [^125^I]-iodide. At 30 min after injection, the intact [^125^I]-4 in the urine reduced to 5%.

SPECT/CT imaging was performed in nude mice bearing KB tumor xenografts after administration of [^125^I]-4 (~5.0 MBq (0.135 mCi)). PMX (400 μg) and/or potassium iodide (4 mg) was injected 1 h before [^125^I]-4 injection. SPECT scans (60 min) were performed ~24 h after injection of [^125^I]-4. The administration of potassium iodide effectively blocked the uptake of radioactivity in the thyroid gland. With preinjection of PMX, renal radioactivity was reduced to background levels. SPECT/CT scans of a mouse that received both potassium iodide and PMX before injection of [^125^I]-4 resulted in a radioactivity uptake that was restricted to FR-positive tumor xenografts, and only traces of radioactivity were observed in non-targeted organs and tissues.

Ex vivo autoradiography of a mouse that received PMX showed that the radioactivity uptake of [^125^I]-4 in the tumor and kidneys decreased to 56% and 4% of the uptake in the control animals, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Reber J., et al. (2012). Radioiodinated Folic Acid Conjugates: Evaluation of a Valuable Concept To Improve Tumor-to-Background Contrast. Mol Pharm.
2 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
3 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
4 Ke C.Y., Mathias C.J., Green M.A. (2004). Folate-receptor-targeted radionuclide imaging agents. Adv Drug Deliv Rev.
5 Konda S.D., et al. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. MAGMA.
6 Low P.S., Henne W.A., Doorneweerd D.D. (2008). Discovery and development of folic-acid-based receptor targeting for imaging and therapy of cancer and inflammatory diseases. Acc Chem Res.
7 Muller C., et al. (2011). Tumor targeting using 67Ga-DOTA-Bz-folate--investigations of methods to improve the tissue distribution of radiofolates. Nucl Med Biol.
8 Tarli L., et al. (1999). A high-affinity human antibody that targets tumoral blood vessels. Blood.